# N-4-[^18^F]Fluorobenzoyl-c[(RGDyK)]_2_

Chemical name: | N-4-[^18^F]Fluorobenzoyl-c[(RGDyK)]_2_
Abbreviated name: | [^18^F]FB-c[(RGDyK)]_2_, [^18^F]FB-RGD_2_
Synonym:
Agent Category: | Peptide
Target: | Integrin α_v_β_3_
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FRGD2)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell-cell and cell-matrix interactions (1). They consist of an α and a β subunit and are important for cell adhesion and signal transduction. α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. α_v_β_3_ antagonists are being studied as antitumor and antiangiogenic agents and the agonists as angiogenic agents for coronary angiogenesis (6, 8, 9). A tripeptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Most of the cyclic RGD peptides are monomeric and are composed of five amino acids. [^18^F]FB-c(RGDyK) was synthesized to study in vivo biodistribution of the tracer in tumor-bearing mice. [^18^F]FB-c(RGDyK) was found to have high accumulation in tumors, but it also had high tumor washout and biliary excretion into the gallbladder and intestines (11). A dimeric analog was synthesized as [^18^F]FB-E[c(RGDyK)]_2_, which was shown to have higher tumor uptake (~1-fold) than the monomer and predominantly renal excretion (12).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FRGD2%20and%20synthesis)]

N-Succinimidyl 4-[^18^F]fluorobenzoate ([^18^F]SFB) was synthesized in two steps from [^18^F]KF in 65 min (11). The decay-corrected yields of [^18^F]SFB were 60-65% based on starting [^18^F]KF. [^18^F]SFB was used to conjugate c(RGDyK) and E[c(RGDyK)]_2_ to form [^18^F]FB-c(RGDyK) and [^18^F]FB-E[c(RGDyK)]_2_, respectively. Radiochemical purities >99% were obtained for both peptides, and radiochemical yields were 35-45% for the monomer and 20-30% for the dimers (11). The specific activity was 222 GBq/μmol (6 Ci/μmol) at end of synthesis. Total synthesis time was about 200 min including the final high-performance liquid chromatography purification.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FRGD2%20and%20%28in%20vitro%20or%20cell%29)]

A receptor-binding assay with ^125^I-c(RGDyK) was established using a primary human brain capillary endothelial cells. FB-c(RGDyK), FB-E[c(RGDyK)]_2_, c(RGDyK), and [c(RGDyK)]_2_ had inhibitory concentrations (IC_50_ values) of 16.9 ± 0.5, 6.7 ± 0.5, 3.5 ± 0.3, and 2.3 ± 0.7 nM, respectively (12).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FRGD2%20and%20rodentia)]

Chen et al. (12) performed biodistribution studies of [^18^F]FB-E[c(RGDyK)]_2_ in nude mice, using a U87MG glioblastoma s.c. xenograft model. Data were obtained at 30 min, 1 h, 2 h, and 4 h after injection. [^18^F]FB-c(RGDyK) had very rapid blood clearance, resulting in very low activity in the blood at 30 min and 4 h (0.81 ± 0.09 and 0.09 ± 0.1% of injected dose (ID)/g, respectively). The initial tracer accumulation in the α_v_β_3_-integrin-expressing U87MG tumor was about 6.8% ID/g at 30 min and decreased to about 2% ID/g at 4 h with a tumor/blood ratio of 23 ± 2. Tumor uptake of radioactivity was significantly and markedly blocked by co-injection of unlabeled c(RGDyK) (10 mg/kg) from 4.27 to 0.45% ID/g. At 1 h, the highest radioactivity was found in the tumor, followed by the kidney, intestine, stomach, lung, and liver. The tracer had very fast renal clearance, with significantly higher kidney accumulation than for the monomer. However, it had lower liver accumulation than the monomer. [^18^F]FB-E[c(RGDyK)]_2_ showed significantly higher accumulation (~1-fold) than the monomer (11). Metabolic studies showed that 80-94% of [^18^F]FB-E[c(RGDyK)]_2_ in the plasma, liver, kidney, and tumor was unchanged at 60 min after injection (13). More than 95% of [^18^F]FB-E[c(RGDyK)]_2_ was intact in the urine. No defluorination of [^18^F]FB-E[c(RGDyK)]_2_ was detected_._

[^18^F]FB-E[c(RGDyK)]_2_ positron emission tomography (PET) imaging of mice bearing U87MG tumors on the right front leg showed that the tumor was clearly visible at 60 min after injection. The tumor/background ratio was 9.5 at 60 min with high uptake also in the kidney, urinary bladder, and gallbladder. Uptake in the tumor, liver, and kidneys was calculated as 4.4, 0.9, and 3.6% ID/g, respectively (11). Tumor uptake of radioactivity was blocked by co-injection of unlabeled c(RGDyK). Further PET studies using mice bearing various experimental tumors with different integrin expression revealed a good linear correlation (R^2^ = 0.96; P = 0.005) between binding potentials (1.9–29.5, calculated from Logan analysis) and the tumor integrin density B_max_ values (determined from in vitro cell-binding assay and ex vivo sodium dodecyl sulfate--polyacrylamide gel electrophoresis followed by autoradiography) (13).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FRGD2%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FRGD2%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FRGD2%20and%20%28human%20not%20cell%29)]

No publication is currently available.

## NIH Support

P50 CA114747, R24 CA93826, R21 EB001785

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
12 Chen X., Tohme M., Park R., Hou Y., Bading J.R., Conti P.S. (2004). Micro-PET imaging of alphavbeta3-integrin expression with 18F-labeled dimeric RGD peptide. Mol Imaging.
13 Zhang X., Xiong Z., Wu Y., Cai W., Tseng J.R., Gambhir S.S., Chen X. (2006). Quantitative PET Imaging of Tumor Integrin {alpha}v{beta}3 Expression with 18F-FRGD2. J Nucl Med.